# ^111^In-Labeled Ac-TZ14011 peptide (a chemokine receptor 4 antagonist) conjugated to CyAL5.5 (a fluorescent dye) through a multifunctional single-attachment point (MSAP) reagent

Chemical name: | ^111^In-Labeled Ac-TZ14011 peptide (a chemokine receptor 4 antagonist) conjugated to CyAL5.5 (a fluorescent dye) through a multifunctional single-attachment point (MSAP) reagent
Abbreviated name: | [^111^In]Ac-TZ14011-MSAP
Synonym:
Agent Category: | Peptide
Target: | Chemokine receptor 4 (CXCR4)
Target Category: | Receptor
Method of detection: | Multimodal (single-photon emission computed tomography (SPECT), gamma planar imaging; optical imaging)
Source of signal / contrast: | ^111^In and CyAL5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-TZ14011%20peptide&cmd=DetailsSearch)]

The chemokine receptor 4 (CXCR4) and its ligand, the stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and hematopoietic systems (1, 2). In addition, these receptor–ligand pairs have a major role in the development, progression, and spread of various cancers (3), and the CXCR4 acts as a co-receptor to facilitate entry of the human immunodeficiency virus (HIV) into CD4^+^ cells (4). It has also been suggested that CXCR4 and SDF-1 participate in the pathogenesis of neurodegenerative and inflammatory conditions (5). The level of CXCR4 expression by tumor cells is considered to play a critical role in cancer metastasis by generating a chemotactic gradient to organs expressing the SDF-1, and the overexpression of CXCR4 in cancerous lesions indicates a poor prognosis for patients suffering from different types of cancer (6). The role of CXCR4 (http://clinicaltrials.gov/ct2/results?term=CXCR4) and SDF-1 (http://clinicaltrials.gov/ct2/results?term=SDF-1) for cancer metastasis is under investigation in several clinical trials approved by the United States Food and Drug Administration.

Because CXCR4 and SDF-1 are considered to play an important role in the development and progression of HIV infections and cancer, researchers have attempted to quantify CXCR4 levels with noninvasive imaging techniques for various pathological and physiological conditions (7). SDF-1 labeled with technetium (^99m^Tc) was used as a probe to determine changes in CXCR4 expression in the heart after a myocardial infarction, and it was concluded that the probe was suitable to visualize expression of the receptor in tissue with single-photon emission computed tomography (SPECT). In another study, copper (^64^Cu)-labeled 1,1'-{1,4-phenylenebis(methylene)}-bis{1,4,8,11-tetraaza-cyclotetradecane} (AMD3100), an inhibitor of CXCR4 activity, was used for imaging and to study the biodistribution of the radiochemical with positron emission tomography in normal mice (8). This study showed that [^64^Cu]AMD3100 accumulated mainly in the liver, kidneys, and spleen of the animals. An indium (^111^In)-labeled CXCR4 antagonist peptide, [^111^In]Ac-TZ14011, discussed in a separate chapter of MICAD (9), was developed for the scintigraphic imaging of xenograft tumors that express CXCR4 in mice, and its biodistribution was also investigated in the animals (10). A dual-imaging (multimodal imaging) probe has been generated by preparing a multifunctional single-attachment point (MSAP) reagent derivative of the Ac-TZ14011 peptide (11).

A characteristic feature of the MSAP reagent is that its structure contains a diethylenetriamine pentaacetic acid residue (for the chelation of a radionuclide such as ^111^In) and a CyAL5.5 fluorescence dye residue (for fluorescence imaging; the excitation and emission maxima of this dye are 615–665 nm and 695–770 nm, respectively, similar to that of the Cy5.5 fluorescence dye). The dual-imaging probe was produced by conjugating the MSAP reagent with the Ac-TZ14011 peptide (Ac-TZ14011-MSAP), and the conjugate was labeled with ^111^In to obtain the multimodal imaging agent ([^111^In]Ac-TZ14011-MSAP) (11). The dual-labeled probe was evaluated for the imaging of xenograft tumors that overexpress the CXCR4 in mice, and its biodistribution was studied in the same animals (11).

### Related Resource Links

Signaling events mediated by CXCR4 (Pathways Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200099&source=NATURE&output-format=graphic&ppage=1&genes_a=7852))

CXCR4 in Online Mendelian Inheritance in Man database (OMIM (http://omim.org/entry/162643))

Chemokine receptor reviews in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=chemokine%20receptors%20review)

Structure (http://www.ncbi.nlm.nih.gov/structure?term=CXCR4&cmd=DetailsSearch) of CXCR4

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DAc-TZ14011-MSAP%20synthesis&cmd=DetailsSearch)]

The synthesis of [^111^In]Ac-TZ14011-MSAP has been described by Kuil et al. (11). The efficiency of the labeling reaction was reported to be >99%. The number of chelating agents and fluorescent dye molecules per molecule of Ac-TZ14011-MSAP, radiochemical purity, specific activity, and stability of the labeled probe were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DAc-TZ14011-MSAP%20in%20vitro%20studies&cmd=DetailsSearch)]

The expression levels of CXCR4 in human breast cancer cell lines MDAMB231 and MDAMB231^CXCR4+^, which were used for some studies, was confirmed with flow cytometry analysis using a commercially available fluorescent anti-CXCR4 antibody (Ab) (11). The MDAMB231^CXCR4+^ cells were observed to have 4.4-fold higher expression of the receptor compared with the control (basal) MDAMB231 cell line. Flow cytometry analysis with Ac-TZ14011-MSAP and the [^111^In]Ac-TZ14011-MSAP peptides yielded results that were similar to those obtained with the anti-CXCR4 Ab. This indicated that the two peptides were comparable to the anti-CXCR4 Ab for the detection of the chemokine receptor.

Using a competition binding assay with MDAMB231^CXCR4+^ cells, the K_d_ values for Ac-TZ14011-MSAP and [^111^In]Ac-TZ14011-MSAP for CXCR4 were determined to be 186.9 nM and 177.1 nM, respectively (11). This indicated that chelation of indium to the Ac-TZ14011-MSAP peptide did not alter its affinity for the CXCR4.

Fluorescence confocal microscopy imaging of MDAMB231^CXCR4+^ cells exposed to Ac-TZ14011-MSAP at 4°C showed that the cells were stained primarily on the cell membrane (the location of the CXCR4 in the cells) (11). This indicated that the probe was suitable for detection of the chemokine receptor expressed on the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DAc-TZ14011-MSAP%20rodentia&cmd=DetailsSearch)]

Tumors expressing CXCR4 were generated in FVB mice (http://www.criver.com/EN-US/PRODSERV/BYTYPE/RESMODOVER/RESMOD/Pages/FVBMouse.aspx) (n = 3 animals) to assess the receptor targeting ability of [^111^In]Ac-TZ14011-MSAP (11). The animals were intravenously injected with 10 MBq (0.37 mCi; 50 μg) of the radiochemical, and SPECT/computed tomography (CT) images of the animals were acquired 24 h later. From the SPECT/CT images, it was clear that there was a high uptake of radioactivity in the tumors. Fluorescence images of the animals were acquired immediately after the SPECT/CT scans (11). The tumors were also visible clearly in the fluorescence images. No blocking studies were reported.

After completion of the imaging session, the mice were euthanized, and all organs of interest were removed to study the biodistribution of [^111^In]Ac-TZ14011-MSAP (11). Radioactivity accumulation in the different organs was determined, and the results were presented as percent of injected dose per gram tissue (% ID/g). Maximum label was detected in the liver (19.46 ± 4.48% ID/g), followed by the kidney (6.89 ± 1.29% ID/g) and the spleen (4.38 ± 1.16% ID/g). All other organs had an uptake of <2% ID/g (e.g., 0.02 ± 0.00% ID/g in brain, 0.29 ± 0.01% ID/g in muscle, and 1.70 ± 0.08 in intestine). Although the uptake of radioactivity in the tumor was not presented, the tumor/muscle (T/M) ratio was reported to be 4.55 ± 0.68, much higher than the T/M ratio of 1.20 ± 0.12 (P < 0.01) for the control 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cells tumors that did not express the CXCR4.

From these studies, the investigators concluded that Ac-TZ14011-MSAP was probably suitable for image-guided surgery applications in rodents (11).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DAc-TZ14011-MSAP%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DAc-TZ14011-MSAP%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=20641260%5Buid%5D&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
2 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
3 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
4 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
5 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
6 Gelmini S., Mangoni M., Serio M., Romagnani P., Lazzeri E. (2008). The critical role of SDF-1/CXCR4 axis in cancer and cancer stem cells metastasis. J Endocrinol Invest.
7 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
8 Jacobson O., Weiss I.D., Szajek L., Farber J.M., Kiesewetter D.O. (2009). 64Cu-AMD3100--a novel imaging agent for targeting chemokine receptor CXCR4. Bioorg Med Chem.
9 Chopra, A., 111In-Labeled diethylenetriamine-pentaacetic acid-Ac-TZ14011. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Hanaoka H., Mukai T., Tamamura H., Mori T., Ishino S., Ogawa K., Iida Y., Doi R., Fujii N., Saji H. (2006). Development of a 111In-labeled peptide derivative targeting a chemokine receptor, CXCR4, for imaging tumors. Nucl Med Biol.
11 Kuil J., Buckle T., Yuan H., van den Berg N.S., Oishi S., Fujii N., Josephson L., van Leeuwen F.W. (2011). Synthesis and evaluation of a bimodal CXCR4 antagonistic peptide. Bioconjug Chem.